# (R)-3-[^18^F]Fluoro-2-methyl-2-N-(methylamino)propanoic acid

Chemical name: | (R)-3-[^18^F]Fluoro-2-methyl-2-N-(methylamino)propanoic acid
Abbreviated name: | (R)-[^18^F]NMeFAMP
Synonym:
Agent category: | Compound
Target: | L-type and A-type amino acid transporter
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FAMP)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (4-6).The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher metabolic pathways, including incorporation into proteins, than most normal cells (4). L-[^11^C]Methionine and [^18^F]fluorotyrosine have been widely used in the detection of tumors. On the other hand, the non-natural amino acids are not metabolized. Their uptakes are through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can accumulate intracellularly in high concentrations. [^11^C]Aminoisobutyric acid was shown to have a high tumor/background ratio (8, 9). (R)-3-[^18^F]Fluoro-2-methyl-2-N-(methylamino)propanoic acid ((R)-[^18^F]NMeFAMP) is a fluorinated analog of [^11^C]α-aminoisobutyric acid (AIB) that is being evaluated as a useful tracer in PET tumor imaging (10).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20transporter+AND+micad%5Bbook%5D)
- Gene information in NCBI (Amino acid transporter (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=8140))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D)
- Clinical trials (Amino acid transporter (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporter))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+synthesis)]

Nucleophilic fluorination of (R)-3,4-dimethyl-1,2,3-oxathiazolidine-4-carboxylic acid tert-butyl ester 2,2-dioxide with K[^18^F]F/Kryptofix2.2.2 and subsequent hydrolysis and purification provided a radiosynthesis yield (decay-corrected) of 66% for (R)-[^18^F]NMeFAMP at the end of bombardment (10). A radiochemical purity of 99% was obtained. The total synthesis time was 85 min. The specific activity was ~1.85 GBq/µmol (50 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+in+vitro)]

(R)-[^18^F]NMeFAMP exhibited a rapidly increasing uptake into L9 rat gliosarcoma tumor cells with 7.08 ± 0.47% (n = 3) injected dose (ID)/5 × 10^5^ cells at 30 min of incubation (10). The uptake was blocked by the presence of L-type transporter inhibitor BCH (2-amino-bicyclo[2.2.1]heptane-2-carboxylic acid), A-type transporter inhibitor MeAIB (N-methyl-AIB), and system ASC inhibitor ACS (alanine-cysteine-serine) with 54%, 92%, and 89% inhibition, respectively. (S)-[^18^F]NMeFAMP (3.87 ± 0.22% ID/5 × 10^5^ cells) exhibited a lower uptake than (R)-[^18^F]NMeFAMP. The uptake was blocked by the presence of BCH, MeAIB, and ACS with 29%, 79%, and 58% inhibition, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+rodentia)]

Yu et al. (10) performed ex vivo biodistribution studies of (R)-[^18^F]NMeFAMP in rats (n = 5) implanted intracerebrally with a 9L gliosarcoma. The uptake in the brain (0.04% ID/g) was low at 30 min after injection and decreased slightly to 0.02% ID/g at 120 min. The uptake in the tumor was 1.46% ID/g at 15 min and increased to 2.78% ID/g at 120 min after injection. Most of the other tissues showed lower radioactivity levels at 120 min than at 15 min. The tissues with the highest accumulation at 30 min were the pancreas (2.72% ID/g) and kidney (8.91% ID/g). The tumor/brain ratios were 25.0, 53.2, 58.2, and 115.4 at 15, 30, 60, and 120 min, respectively. The radioactivity in the bone was low (0.44% ID/g at 120 min). (S)-[^18^F]NMeFAMP exhibited lower tumor accumulation but slightly higher pancreas and kidney accumulation than (R)-[^18^F]NMeFAMP. The tumor/brain ratios were 20.4, 30.2, 28.7, and 35.4 at 15, 30, 60, and 120 min, respectively. No blocking experiments were performed. The specificity of uptake, especially given the disruption of the blood brain barrier, was not studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FAMP+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FAMP%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Conti P.S., Sordillo P.P., Schmall B., Benua R.S., Bading J.R., Bigler R.E., Laughlin J.S. (1986). Tumor imaging with carbon-11 labeled alpha-aminoisobutyric acid (AIB) in a patient with advanced malignant melanoma. Eur J Nucl Med.
9 Fross R.D., Warnke P.C., Groothuis D.R. (1991). Blood flow and blood-to-tissue transport in 9L gliosarcomas: the role of the brain tumor model in drug delivery research. J Neurooncol.
10 Yu W., McConathy J., Williams L., Camp V.M., Malveaux E.J., Zhang Z., Olson J.J., Goodman M.M. (2010). Synthesis, radiolabeling, and biological evaluation of (R)- and (S)-2-amino-3-[(18)F]fluoro-2-methylpropanoic acid (FAMP) and (R)- and (S)-3-[(18)F]fluoro-2-methyl-2-N-(methylamino)propanoic acid (NMeFAMP) as potential PET radioligands for imaging brain tumors. J Med Chem.